# ^99m^Tc-Human β-defensin-3

Chemical name: | ^99m^Tc-Human β-defensin-3
Abbreviated name: | ^99m^Tc-HBD-3
Synonym:
Agent category: | Peptide
Target: | Microbial membrane
Target category: | Bacteria
Method of detection: | Single-photon emission computed tomography (SPECT), gamma planar imaging
Source of signal\contrast: | ^99m^Tc
Activation: | No
Studies: | - In vitro; - Rodents | Click on protein (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=retrieve&dopt=full_report&list_uids=768&log$=databasead&logdbfrom=protein), nucleotide (http://www.ncbi.nlm.nih.gov/nucleotide/169636419) (RefSeq), and gene (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=ShowDetailView&TermToSearch=55894&ordinalpos=1&itool=EntrezSystem2.PEntrez.Gene.Gene_ResultsPanel.Gene_RVDocSum) for more information about human β-defensin-3.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=defensin-3)]

Antimicrobial peptides are small, cationic, amphiphilic peptides of 12–50 amino acids with microbicidal activity against both bacteria and fungi (1). The mammalian defensins can be subdivided into three main classes according to their structural differences: α-defensins, β-defensins, and theta-defensins. Mammalian α-defensins are predominantly found in neutrophils and in small intestinal epithelial cells, whereas mammalian β-defensins have been isolated from both leukocytes and epithelial cells. Recently, two novel human β-defensins (human β-defensin-3 (HBD-3) and human β-defensin-4 (HBD-4)) have been identified. Similar to HBD-1 and HBD-2, HBD-3 has microbicidal activity toward the Gram-negative bacteria (e.g., Pseudomonas aeruginosa, Escherichia coli) and yeasts. In addition, HBD-3 kills Gram-positive bacteria such as Streptococcus pyogenes or Staphylococcus aureus, including multi-resistant S. aureus strains. In contrast to HBD-1 and HBD-2, significant expression of HBD-3 has been demonstrated in non-epithelial tissues such as leukocytes, heart, and skeletal muscle. HBD-4 is expressed in certain epithelial cells and in neutrophils.

A variety of radiolabeled compounds, including ^67^Ga-citrate, ^99m^Tc-ciprofloxacin, ^18^F-FDG, and ^111^In- or ^99m^Tc-labeled antibodies that interact with specific receptors on the infiltrating leukocytes, and peptides have been evaluated for the detection of infections (2, 3). However, because they accumulate in both infected and inflamed areas of the body, these radiopharmaceuticals are nonspecific and cannot distinguish between infection and inflammation. In an effort to identify and develop radioactive compounds that are specific for the detection of infections, various investigators have evaluated the use of antimicrobial peptides that are found naturally in most multicellular organisms (4). Such peptides bind specifically to microbes, presumably through cationic domains that interact with anionic regions of the microbial membrane, and have been shown to distinguish infected tissue from inflamed tissue (5). Liberatore et al. (6) radiolabeled HBD-3 with ^99m^Tc for single-photon emission computed tomography imaging of infected tissue.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20defensin-3+synthesis)]

A solution Na^99m^TcO_4_ (74–148 MBq (2–4 mCi)) and sodium borohydride in the presence of carbon monoxide was heated for 20 min at 100°C in a vial (6). A solution of HBD-3 (0.020–0.0040 mg) was added to the reaction vial and incubated for 60 min at room temperature (7). ^99m^Tc-HBD-3 was purified with PD-10 column chromatography. The specific activity of the purified product was 2–6 GBq/mg (0.054–0.162 Ci/mg) with a radiolabeling efficiency of 40–50%.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20defensin-3+in+vitro)]

S. aureus and E. coli suspensions were incubated with 2.5–5.0 µg/ml ^99m^Tc-HBD-3, which exhibited ~3-fold higher inhibition of the growth of S. aureus than E. coli (6).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20defensin-3+%20rodentia)]

Liberatore et al. (6) performed ex vivo biodistribution studies of 1.6–3.3 µg ^99m^Tc-HBD-3 in rats with S. aureus infection in the right foreleg and sterile inflammation in the left foreleg (n = 3/group) at 1, 3, and 5 h after injection. Accumulation of radioactivity at the infection sites was 0.053% injected dose/g (ID/g) at 1 h, 0.080% ID/g at 3 h, and 0.083% ID/g at 5 h. Accumulation of radioactivity at the inflammation sites was 0.064% ID/g at 1 h, 0.032% ID/g at 3 h, and 0.033% ID/g at 5 h. Therefore, there was 1.5-fold higher ^99m^Tc-HBD-3 accumulation at the infection sites than at the inflammation sites at 3 h and 5 h after injection. Accumulation in the normal muscle was 0.030–0.036% ID/g at these time points. No blocking experiment was performed. Concentration levels of ^99m^Tc-HBD-3 in blood from mice with infection and inflammation were not reported.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20defensin-3+and%20%28pig%20or%20dog%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20defensin-3+and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=99mTc%20defensin-3+human)]

No publication is currently available.

## References

1 Schneider J.J., Unholzer A., Schaller M., Schafer-Korting M., Korting H.C. (2005). Human defensins. J Mol Med.
2 Boerman O.C., Rennen H., Oyen W.J., Corstens F.H. (2001). Radiopharmaceuticals to image infection and inflammation. Semin Nucl Med.
3 Lupetti A., Nibbering P.H., Welling M.M., Pauwels E.K. (2003). Radiopharmaceuticals: new antimicrobial agents. Trends Biotechnol.
4 Welling M.M., Lupetti A., Balter H.S., Lanzzeri S., Souto B., Rey A.M., Savio E.O., Paulusma-Annema A., Pauwels E.K., Nibbering P.H. (2001). 99mTc-labeled antimicrobial peptides for detection of bacterial and Candida albicans infections. J Nucl Med.
5 Dhople V., Krukemeyer A., Ramamoorthy A. (2006). The human beta-defensin-3, an antibacterial peptide with multiple biological functions. Biochim Biophys Acta.
6 Liberatore M., Pala A., Scaccianoce S., Anagnostou C., Di Tondo U., Calandri E., D'Elia P., Gross M.D., Rubello D. (2009). Microbial Targeting of 99mTc-Labeled Recombinant Human {beta}-Defensin-3 in an Animal Model of Infection: A Feasibility Pilot Study. J Nucl Med.
7 Zhao M., Li Z., Bugenhagen S. (2008). 99mTc-labeled duramycin as a novel phosphatidylethanolamine-binding molecular probe. J Nucl Med.